# [2-[^18^F]Fluoromethoxy-5-(5-trifluoromethyl-tetrazol-1-yl)-benzyl]([2S,3S]2-phenyl-piperidin-3-yl)-amine

Chemical name: | [2-[^18^F]Fluoromethoxy-5-(5-trifluoromethyl-tetrazol-1-yl)-benzyl]([2S,3S]2-phenyl-piperidin-3-yl)-amine
Abbreviated name: | [^18^F]SPA-RQ
Synonym: | [^18^F]Substance-P antagonist-Receptor quantifier[^18^F]L-829
Agent Category: | Compound
Target: | NK_1_ receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Other non-primate mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DSPA-RQ%20OR%20%28NK1%20PET%20ligand%29)]

[2-[^18^F]Fluoromethoxy-5-(5-trifluoromethyl-tetrazol-1-yl)-benzyl]([2S,3S]2-phenyl-piperidin-3-yl)-amine ([^18^F]SPA-RQ) is a radioligand developed for positron emission tomography (PET) imaging of NK_1_ receptors (SP receptors) in the central nervous system (CNS) (1).

Tachykinins are 10-12 amino acid peptides that share a common carboxy-terminal sequence “Phe-X-Gly-Leu-Met-amide” where “X” is different but always a hydrophobic residue that is either an aromatic or a beta-branched aliphatic (2-4). This peptide family consists of substance P (SP), neurokinin A (NK_A_), and neurokinin B (NK_B_). The tachykinin peptides mediate their effects by specific G protein coupled receptors. These receptors are divided into three subtypes: neurokinin 1 (NK_1_, formerly the SP receptor), neurokinin 2 (NK_2_, formerly the substance K/substance E receptor/NK-A receptor), and neurokinin 3 (NK_3_, formerly the NK-B receptor) receptors. The effects of SP are mediated primarily via the NK_1_ receptor subtypes. There is evidence that SP behaves like a neurotransmitter involved in regulation of emotional and behavioral responses to a range of noxious and stressful stimuli (5). SP may also play a role in neurogenic inflammation, vasomotor control, and many gastrointestinal functions. Studies have shown that in the brain SP is found throughout the neocortex, in limbic areas, habenula, periaqueductal gray, midbrain nuclei, and especially enriched in the basal ganglia. There is little SP in the cerebellum. The distribution of the NK_1_ receptors in the brain generally corresponds to that of SP.

SP-NK_1_ receptor pathways are found in both CNS and peripheral nervous system. The CNS pathways have been implicated in the pathophysiology of pain, nausea/emesis, and depression disorders (6). PET and single-photon emission tomography of radioligands targeting NK_1_ receptors can visualize and study the CNS NK_1_ receptors in normal and pathologic states. These studies can identify the degree of receptor occupancy in patients with depression and the change in response to therapy (6). A number of NK_1_ selective agonists and antagonists have been successfully labeled, but they failed to provide a specific signal in vivo (1, 6). Solin et al (1). developed a selective NK_1_ receptor antagonist, SPA-RQ, with a high affinity for NK_1_ receptor (IC_50_ = 67 pM) and moderate lipophilicity (logP = 1.8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSPA-RQ%20OR%20%28PET%20NK1%20ligand%29%29%20AND%20synthesis%5BAll%20Fields%5D)]

Solin et al. (1) reported the synthesis and characterization of [^18^F]SPA-RQ. The precursors were prepared either as [2-hydroxy-5-(5-trifluoromethyl-tetrazol-1-yl)-benzyl]([2S,3S]2-phenyl-piperidin-3-yl)-amine hydrochloride or (2S,3S)-1-t-butoxycarbonyl-2-phenyl-3-[2-hydroxy-5-(5’-rifluoromethyltetrzol-1-yl)phenylmethyleneamino]piperidine. The first precursor gave very low and unreliable yields. The second precursor with a tert-butoxycarbonyl (t-BOC) protecting group was prepared from 2-hydroxy-5-(5-trifluoromethyl-tetrazol-1-yl)-benzaldehyde in two steps. In a five-step method of radiosynthesis, [^18^F]FCH_2_Br was first synthesized from dibromomethane via a nucleophilic substitution with [^18^F]F−. [^18^F]F− was obtained from the nuclear reaction ^18^O(p,n)^18^F, and the target water was removed by azeotropic distillations. Dibromomethane in acetonitrile was added to produce [^18^F]FCH_2_Br with about 40% yield (decay corrected to the end of bombardment). [^18^F]FCH_2_Br was used to [^18^F]fluoroalkylate the deprotonated phenolic hydroxyl group of the precursor by bubbling through the precursor solution in dimethylformamide (DMF) and cesium carbonate. The reaction mixture was heated at 110 ºC for 8 min. After DMF was removed, trifluoroacetic acid was added for a 2-min hydrolysis at room temperature to cleave the t-BOC protecting group. The resulting [^18^F]SPA-RQ was purified by preparative high performance liquid chromatography. The radiochemical yield was 9.6 ± 4.0% (n = 111), and the radiochemical purity was 99.5 ± 0.2%. The specific activity was 1190 ± 1310 GBq (32 ± 35.4 Ci)/μmol at the end of synthesis. The total synthesis time was about 60 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSPA-RQ%20OR%20%28PET%20NK1%20ligand%29%29%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

Hietala et al. (2) conducted postmortem human brain receptor autoradiography with [^18^F]SPA-RQ by incubating three left cerebral hemispheres with 50 pM [^18^F]SPA-RQ (specific activity ≥ 400 GBq (10.8 Ci)/μmol) for 60 min at room temperature. Nonspecific binding was estimated by competing the radiotracer binding with 1 mM excess of an unlabeled specific high-affinity NK_1_ receptor antagonist (GR203040). The relative radioactivity concentrations were highest in striatum > cortical regions = thalamus > cerebellum. The addition of GR203040 prevented radioactivity localization almost completely in caudate, putamen, and occipital cortical areas with %blockade of 98 ± 2, 94 ± 2, and 95 ± 4, respectively. The cerebellar radioactivity level was not affected by GR203040 because there was minimal NK_1_ receptor present.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DSPA-RQ%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSPA-RQ%20OR%20%28PET%20NK1%20ligand%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Solin et al. (1) injected [^18^F]SPA-RQ into 4 guinea pigs. Two animals (animal 3 and 4) were pretreated with a NK_1_ selective antagonist (2 mg/kg) 2 min before the administration. The animals were sacrificed at 180 min after injection, and brains were removed for assay. The radiotracer showed a high radioactivity localization in the caudate/putamen, moderate radioactivity in the cortex, and low radioactivity in the cerebellum. For the untreated animals, animal 1 and 2, the ratios of caudate/putamen were 14 and 7.1, respectively. Their ratios of cortex to cerebellum were 4.7 and 2.7, respectively. In comparison, these cortex/cerebellum ratios in the pretreated animal 3 and 4 were ranging from 1.0 to 1.3.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSPA-RQ%20OR%20%28PET%20NK1%20ligand%29%29%20AND%20%28primate%20NOT%20human%29)]

Hargreaves (6) reported that the highest [^18^F]SPA-RQ radioactivity concentration was in the caudate of the monkey brain. In the cerebellum, the radioactivity was washed out with time. Pretreatment with an unlabeled SP antagonist decreased ^18^F]SPA-RQ radioactivity in the caudate and cortex, but no effect was observed in the cerebellum.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DSPA-RQ%20OR%20%28PET%20NK1%20ligand%29%29%20AND%20human)]

PET imaging with [^18^F]SPA-RQ was performed in 10 healthy male volunteers (2). Each subject received i.v. 125-135 MBq (3.38-3.65 mCi) of [^18^F]SPA-RQ (average specific activity = 1,995 GBq (53.9 Ci)/μmol; 114 ng). There was a rapid radioactivity localization in the brain with the highest radioactivity levels in the putamen and caudate nucleus. The cerebellum level was the lowest as the radioactivity was washed out readily. The neocortex and thalamus radioactivity levels were between the striatal level and cerebellar level. The highest putamen/cerebellum and caudate/cerebellum ratios were between 5 and 6 at 215 min and 225 min, respectively. Based on the reference tissue input model, the NK_1_ binding potentials (n = 4) were 5.24 ± 0.40 (caudate), 5.72 ± 0.33 (putamen), 2.60 ± 0.60 (ventral midbrain), 2.60 ± 0.54 (posterior cingulated cortex), and 2.60 ± 0.13 (amygdala). The distribution of [^18^F]SPA-RQ in vivo was similar to the in vitro pattern reported in human brain receptor autoradiography studies. The study suggested that NK_1_ receptors were widely distributed throughout the human brain with highest density in the striatum and visual cortex. Plasma radioactivity analysis by planar chromatography and digital autoradiography indicated that about 30-40% of [^18^F]SPA-RQ remained unchanged at 80 min. Unidentified hydrophilic metabolites and free fluoride were found in these plasma samples.

## References

1 Solin O, Eskola O, Hamill TG, Bergman J, Lehikoinen P, Gronroos T, Forsback S, Haaparanta M, Viljanen T, Ryan C, Gibson R, Kieczykowski G, Hietala J, Hargreaves R, Burns HD. (2004). Synthesis and characterization of a potent, selective, radiolabeled substance-P antagonist for NK1 receptor quantitation: ([18F]SPA-RQ). Mol Imaging Biol.
2 Hietala J, Nyman MJ, Eskola O, Laakso A, Gronroos T, Oikonen V, Bergman J, Haaparanta M, Forsback S, Marjamaki P, Lehikoinen P, Goldberg M, Burns D, Hamill T, Eng WS, Coimbra A, Hargreaves R, Solin O. (2005). Visualization and quantification of neurokinin-1 (NK1) receptors in the human brain. Mol Imaging Biol.
3 Severini C, Improta G, Falconieri-Erspamer G, Salvadori S, Erspamer V. (2002). The tachykinin peptide family. Pharmacol Rev.
4 Datar P, Srivastava S, Coutinho E, Govil G. (2004). Substance P: structure, function, and therapeutics. Curr Top Med Chem.
5 Mantyh PW Neurobiology of substance P and the NK1 receptor J Clin Psychiatry 2002 63Suppl 116 10 12562137
6 Hargreaves R Imaging substance P receptors (NK1) in the living human brain using positron emission tomography J Clin Psychiatry 2002 63Suppl 1118 24 12562139